# Iron oxide–ferritin nanocages

Chemical name: | Iron oxide–ferritin nanocages
Abbreviated name: | Fn-Fe nanocages
Synonym:
Agent category: | Polypeptide nanoparticle
Target: | Non-targeted
Target category: | Non-targeted
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ferritin%20nanoparticle)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the nuclear density (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide nanoparticles and other iron oxide formulations affect T2 primarily and lead to a decreased signal. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

Endothelial cells are important cells in inflammatory responses (2, 3). Bacterial lipopolysaccharides, viruses, inflammation, and tissue injury increase secretion of tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokines and chemokines. Emigration of leukocytes from blood is dependent on their ability to adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell-surface adhesion molecules, such as intracellular adhesion molecule-1, vascular cell adhesion molecule-1, integrins, and selectins. Chemokines are chemotactic to inflammatory cells (such as leukocytes and macrophages) attracting them to sites of inflammation and tissue injury. Under atherogenic conditions, deposition of lipids on the endothelial cell surfaces of the aorta and inflammatory cells leads to the development of atherosclerotic plaques (4), which may erode and rupture.

Ferritin (Fn) is composed of 12 or 24 subunits of heavy and/or light chains, which self-assemble to form a cagelike nanoparticle (nanocage) at physiological pH (7.4) with internal and external diameters of 8 nm and 12 nm for the 24 subunit Fn (5-7), respectively. There are four or eight ion channels for directing Fe^2+^ ions to multiple Fe^2+^/O oxidoreductase (“ferroxidase”) sites in the heavy chains for Fe_2_O_3_•H_2_O deposition in the Fn cavity. The ion channels also control reduction, dissolution, and exit of Fe^2+^ from the mineral with gated pores on the surface of Fn cages. Fe^2+^ ions are required for protein cofactor synthesis and anti-oxidant activity after stress. Most ferritins are intracellular and tissue-specific. For applications, the outer surface of Fn can be chemically or genetically modified with ligands, and the cavity of Fn can capture metal ions with high affinity (8). Uchida et al. (9) loaded iron oxide into the cavities of human heavy chain Fn (Fn-Fe) nanocages to study the in vitro uptake of Fn-Fe nanocages by macrophages. Fn-Fe nanocages have been studied for MRI of vascular macrophages in atherosclerotic plaques in mice (10).

### Related Resource Links:

- Chapters in MICAD (Ferritin (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Ferritin+AND+micad%5Bbook%5D))
- Gene information in NCBI (Ferritin heavy chain (http://www.ncbi.nlm.nih.gov/gene/2495), ferritin light chain (http://www.ncbi.nlm.nih.gov/gene/2512))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Ferritin heavy chain (http://www.ncbi.nlm.nih.gov/omim/134770), ferritin light chain (http://www.ncbi.nlm.nih.gov/omim/134790))
- Clinical trials (Ferritin (http://www.clinicaltrials.gov/ct2/results?term=ferritin))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ferritin%20nanoparticle+synthesis)]

Recombinant human Fn subunits (heavy chains) were purified from transfected Escherichia coli cell lysates. For cage mineralization, ammonium iron(II) sulfate hexahydrate (12.5 mM) and hydrogen peroxide (4.17 mM) solutions (7.9 ml each) were added simultaneously to a solution (10 ml) of Fn nanocages (19.8 nmol, pH 8.5) over a period of ~50 min at 65°C (9). After the mineralization procedure, sodium citrate (60 mmol) was added to chelate any remaining free Fe. After dialysis, Fn-Fe nanocages were purified with column chromatography. There were ~3,000-5,000 Fe molecules per nanocage. The diameters of Fn-Fe nanocages were determined with dynamic light scattering and transmission electron microscopy (TEM) to be 13.5 nm and 12 nm, respectively. The average size of iron oxide particles inside the cage was determined with TEM to be 5.9 ± 0.9 nm. R1 and R2 relaxivity values (1.5 T) of Fn-Fe nanocages were 8.4 mM^-1^s^-1^ and 93 mM^-1^s^-1^, respectively. These values were similar to those of Ferumoxides (http://www.ncbi.nlm.nih.gov/pubmed/20641244) and Ferumoxtran-10 (http://www.ncbi.nlm.nih.gov/pubmed/20641603).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ferritin%20nanoparticle+in%20vitro)]

Uchida et al. (9) performed cellular uptake studies of Fn-Fe nanocages (0.165 mg Fe/ml), Ferumoxides (0.165 mg Fe/ml), and Ferumoxtran-10 (0.165 mg Fe/ml) in murine macrophage cells (RAW). Internalization of Fn-Fe nanocages by RAW cells was similar to that of Ferumoxides as measured with Prussian blue staining of Fe after 24 h of incubation, whereas Ferumoxtran-10 showed little staining at the same time point. Quantitative analysis of Fe uptake as measured with inductively coupled plasma mass spectrometry showed that cellular uptake values were 116 pg Fe/cell, 152 pg Fe/cell, and 3 pg Fe/cell at 72 h of incubation for Fn-Fe nanocages, Ferumoxides, and Ferumoxtran-10, respectively. There were slight decreases (~10%) in cell viability of treated RAW cells, but these decreases were not statistically significant (P > 0.05).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ferritin%20nanoparticle+rodentia)]

Terashima et al. (10) performed MRI (7 T) of macrophages in atherosclerotic carotid arteries in streptozotocin (STZ)-induced diabetic mice. At day 14 after STZ injection, the left common carotid artery (LCA) was ligated in 5 mice and sham-operated in 3 mice. Fn-Fe nanocages (25 mgFe/kg) were injected intravenously. MRI images of both LCA and right common carotid artery (RCA) were obtained at 24 h and 48 h after injection. There was a clear T2* signal loss in the macrophage-rich ligated LCA, but not in the control RCA or in either artery in sham-operated mice. Quantitative analysis showed that the T2*-induced reduction in lumen contrast was significant at both 24 h and 48 h in the ligated LCA compared to contralateral RCA and sham controls (P < 0.01). Immunohistochemical analysis showed macrophage infiltration in the ligated LCA but not in the non-ligated RCA. Fn-Fe nanocages were co-localized with macrophages in the neointima of the ligated LCA but not in the RCA or sham-operated arteries.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ferritin%20nanoparticle+and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ferritin%20nanoparticle+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ferritin%20nanoparticle+human)]

No publication is currently available.

## NIH Support

R01 HL078678, R21 EB005364

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
3 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
4 Libby P. (2002). Inflammation in atherosclerosis. Nature.
5 Maham A., Tang Z., Wu H., Wang J., Lin Y. (2009). Protein-based nanomedicine platforms for drug delivery. Small.
6 Uchida M., Kang S., Reichhardt C., Harlen K., Douglas T. (2010). The ferritin superfamily: Supramolecular templates for materials synthesis. Biochim Biophys Acta.
7 Theil E.C. (2011). Ferritin protein nanocages use ion channels, catalytic sites, and nucleation channels to manage iron/oxygen chemistry. Curr Opin Chem Biol.
8 Uchida M., Flenniken M.L., Allen M., Willits D.A., Crowley B.E., Brumfield S., Willis A.F., Jackiw L., Jutila M., Young M.J., Douglas T. (2006). Targeting of cancer cells with ferrimagnetic ferritin cage nanoparticles. J Am Chem Soc.
9 Uchida M., Terashima M., Cunningham C.H., Suzuki Y., Willits D.A., Willis A.F., Yang P.C., Tsao P.S., McConnell M.V., Young M.J., Douglas T. (2008). A human ferritin iron oxide nano-composite magnetic resonance contrast agent. Magn Reson Med.
10 Terashima M., Uchida M., Kosuge H., Tsao P.S., Young M.J., Conolly S.M., Douglas T., McConnell M.V. (2011). Human ferritin cages for imaging vascular macrophages. Biomaterials.